# ^111^In-Diethylenetriaminepentaacetic acid-polyethylene glycol-annexin V

Chemical name: | ^111^In-Diethylenetriaminepentaacetic acid-polyethylene glycol -annexin V
Abbreviated name: | ^111^In-DTPA-PEG-Anx5
Synonym: | ^111^In-PEGylated annexin V, ^111^In-DTP-Anx5
Agent Category: | Protein
Target: | Phosphatidylserine (PS)
Target Category: | Specific binding
Method of detection: | SPECT (Single Photon Emission Computed Tomography), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=430966), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4809273) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=308) for more information about Annexin V

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-annexin%20V%29%20OR%20%28111I-DTPA-PEG-annexin%20V%29)]

^111^In-Diethylenetriaminepentaacetic acid-polyethylene glycol-annexin V (^111^In-DTPA-PEG-Anx5) is a radiolabeled protein developed for single-photon emission computed tomography (SPECT) imaging of programmed cell death (apoptosis) (1, 2). ^111^In is a gamma emitter with a physical t_½_ of 2.8 days.

Apoptosis is an essential biological process that maintains homeostasis of tissues and organs in concert with proliferation, growth, and differentiation (3, 4). Cell death can occur by the process of necrosis or by the process of apoptosis. Apoptosis is a highly regulated, genetically controlled, noninflammatory process requiring ATP (5). The apoptotic process can be triggered either by a decrease in factors required to maintain the cell in good health or by an increase in factors that cause cells to die (6). The two known mechanisms of apoptosis are the death receptor (extrinsic) and the mitochondrial (intrinsic) pathways (7). Annexin V (Anx5) is one of the numerous members of the calcium- and phospholipid-binding superfamily of annexin proteins. The mature Anx5 molecule consists of 319 amino acids with a total molecular weight of 35.8 kDa. Most of the biological functions of Anx5 are based on its high affinity for negatively charged phospholipids in the presence of physiologic concentrations of calcium. Anx5 binds to membrane-bound phophatidylserine (PS) which is normally restricted to the inner leaflet of the plasma membrane lipid bilayer (6). PS is exposed on the surfaces of cells as they undergo apoptosis. This change in the membrane can be detected by the binding of Anx5 to the external PS (7-9). It is also possible that Anx5 binds to PS exposed on the cell surface in pathologic conditions associated with necrosis and vascular damage. As a result, PS-targeting is not entirely specific to apoptotic cell death. In vivo imaging using radiolabeled Anx5 does not discriminate between apoptotic and necrotic cell death (7).

Anx5 has been labeled with various radionuclides for SPECT and positron emission tomography imaging of apoptosis (7, 10). The detection of cell death in vivo has potential clinical value for possible diagnosis and assessment of therapeutic efficacy in transplanted organ rejections, AIDS, septic shock, cardiovascular diseases, neurodegenerative disorders, and cancer. Ke et al. (11) hypothesized that radiolabeled Anx5 with sufficiently long t_½_ would allow tumor imaging with deeper penetration into the tumor mass and would capture a more complete picture of the dynamic process of the apoptotic cell generation and removal (7). Based on the ^111^In-DTPA-PEG (^111^In-diethylenetriaminepentaacetic acid-polyethylene glycol) conjugation method developed by Wen et al. (12), Ke et al. (11) and Wen et al. (13). Anx5 radiolabeled with ^111^In for imaging of tumor apoptosis. The introduction of an uncharged, amphiphilic linear polymer (PEG) to protein molecules appeared to improve their biocompatibility, increase circulation t_½_, decrease immunogenicity, increase resistance to proteolysis, and enhance solubility and stability (14). PEG modification also reportedly interfered with the recognition of foreign particles and proteins by the reticuloendothelial system and reduced the liver uptake.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28111In-annexin%20V%29%20OR%20%28111I-DTPA-PEG-annexin%20V%29%29%20AND%20synthesis)]

Wen et al. (14) discussed the preparation of a heterfunctional PEG with one end attached to the radiometal chelator, DTPA , and the other end attached to the protected thiol group, S-acetylthioacetate (S-ATA). This allowed the simultaneous introduction of both a metal-chelating agent and the PEG molecule to the protein molecule and avoided excessive modification of the protein molecule. Briefly, DTPA-PEG-NH_2_ was prepared by adding t-Boc-NH-PEG-NH_2_ to a stirred suspension of DTPA-dianhydride and triethylamine (TEA) in chloroform at room temperature for 2 h. The t-Boc protecting group was then removed by adding trifluoroacetic acid at room temperature for 4 h. DTPA-PEG-NH_2_ was then reacted with S-ATA in chloroform at room temperature for 1 h to produce DTPA-PEG-ATA. DTPA-PEG-ATA can conjugate with any maleimide-activated proteins. Wen et al. (13) further improved this technique by introducing an NH_2_-reactive isothiocyanate (SCN−) functional group in place of the ATA. This eliminated the required maleimide-activation of the protein molecules. In this improved method, p-NO_2_-benzoyl-PEG-DTPA was produced by reacting DTPA-PEG-NH2 with p-nitrobenzoyl chloride and TEA in chloroform for 4 h with a yield of 90%. The resulting p-NO_2_-benzoyl-PEG-DTPA was then mixed with 10% Pd/C in water under 35 psi H_2_ overnight to produce p-NH_2_-benzoyl-PEG-DTPA. This compound was reacted with thiophosgene in chloroform at room temperature for 2 h to give p-SCN-benzoyl-PEG-DTPA with a yield of 95%. The molecular weight of p-SCN-benzoyl-PEG-DTPA was estimated to be 81-114 kDa and each PEGylated Anx molecule contained approximately 10-16 PEG molecules.

The radiosynthesis of ^111^In-PEG-Anx5 involved adding 0.09 μmol p-SCN-benzoyl-PEG-DTPA to 0.006 μmol Anx5 (15:1 ratio of DTPA-PEG to Anx5) in 0.1M sodium phosphate buffer and stirred at 4ºC overnight (13). After purification by anionic ion exchange column, DTPA-PEG-Anx5 was incubated with ^111^InCl_3_ in 20 mM Tris buffer for 15 min. ^111^In-Anx5 was purified by gel filtration chromatography to remove unreacted ^111^In. Specific activity was 296-370 kBq (8-10 μCi)/0.028 nmole (based on 35.8 kDa molecular weight) and the radiochemical yield was 91%. Successful preparations of ^111^In-PEG-Anx5 in the 30:1 and 60:1 ratios of DTPA-PEG to Anx5 were also achieved.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28111In-annexin%20V%29%20OR%20%28111I-DTPA-PEG-annexin%20V%29%29%20AND%20in%20vitro)]

Wen et al. (13) reported that ^111^In-PEG-Anx5 was relatively stable in 20% fetal bovine serum at 37ºC. Using high-performance liquid chromatography analysis, the percentages of intact conjugate were 94%, 69%, and 61% at 1 day, 2 days, and 5 days after incubation. Cell binding assays were carried out in human leukemia HL60 cells and human B-cell lymphoma Raji cells. These cells were treated with Ara-C at 1.0 μM for 22 h to induce apoptosis. Flow cytometry analysis using fluorescent Anx5-FITC as a probe showed a good correlation between cell-associated radioactivity of the 30:1 ^111^In-PEG-Anx5 preparation and the percentage of induced apoptotic cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28111In-annexin%20V%29%20OR%20%28111I-DTPA-PEG-annexin%20V%29%29%20AND%20rodentia)]

Wen et al (13) studied the pharmacokinetics and biodistribution of ^111^In-PEG-Anx5 (15:1 preparation) in nude mice. Each mouse received a dose of 2.59 MBq (70 μC i) per 7 μg. The activity-time profile of ^111^In-PEG-Anx5 fitted well into a two-compartment model. The rate of clearance and volume of distribution were 0.01 ml/h and 0.2 ml, respectively. The t_½α_ and t_½β_ values were 4.90 h and 26.3 h, respectively. In comparison, the ^111^In-DTPA-unPEGylated Anx5 had the clearance rate, volume of distribution, and t_½α_ and t_½β_ values of 0.4 ml/h, 6.1 ml, 0.07 h, and 17.4 h, respectively. Biodistribution studies at 120 h after the injection showed that ^111^In-PEG-Anx5 had significantly reduced localization in the kidney and increased activity in the spleen compared with ^111^In-DTPA-unPEGylated Anx5. The percentages of injected dose per gram of tissue (%ID/g, n = 3) for blood, liver, kidney, spleen, and muscle were 0.36 ± 0.05%, 8.37 ± 2.76%, 22.35 ± 4.74%, 6.75 ± 0.44%, and 0.75 ± 0.04%, respectively.

Ke et al. (11) evaluated ^111^In-PEG-Anx5 for tumor imaging in a tumor model of poly(L-glutamic acid)-paclitaxel (a chemotherapeutic agent) and anti-EGR C-225 monoclonal antibody (MAb)-induced apoptosis in mammary MDA-MB-468 tumor-bearing nude mice. Each mouse received a dose of 1.48 MBq (40 μCi) per 4 μg. The radioactivity levels (%ID/g, n = 3) at 48 h after injection in paclitaxel-treated mice (treatment of 4 days) were 4.56 ± 0.64 (blood), 49.24 ± 7.70 (liver), 27.22 ± 4.36 (kidney), 1.21 ± 0.25 (muscle), and 15.99 ± 4.27 (tumor). The tumor radioactivity was 8.13 ± 0.28% ID/g in untreated mice. In comparison, the tumor radioactivity levels of ^111^In-DTPA-unPEGylated Anx5 were 0.62 ± 0.14, 1.23 ± 0.67, for untreated and treated mice, respectively. Histologic analysis of tumor tissues showed a significant correlation (r = 0.87 P = 0.02) between the tumor radioactivity level of ^111^In-PEG-Anx5 and the apoptotic index (percentage of apoptotic nuclei induced by drug treatment). Autoradiograms of tumor tissues showed that the radioactivity of ^111^In-PEG-Anx5 was localized in the central zone as well as in the periphery. In comparison, the radioactivity of ^111^In-DTPA-unPEGylated Anx5 was mainly confined to the periphery. Intense TUNEL (DNA fragmentation) staining corresponded to hot spots from ^111^In-PEG-Anx5. Gamma imaging was able to clearly visualize the changes in tumor radioactivity levels of ^111^In-PEG-Anx5 in treated mice. ^111^In-DTPA-unPEGylated Anx5 did not reveal the tumors in either treated or untreated mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28111In-annexin%20V%29%20OR%20%28111I-DTPA-PEG-annexin%20V%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28111In-annexin%20V%29%20OR%20%28111I-DTP%28A-PEG-annexin%20V%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28111In-annexin%20V%29%20OR%20%28111I-DTP%28A-PEG-annexin%20V%29%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIH 9081001, NIH Cancer Center Support Grant CA16672, NIH U54 CA090810.

## References

1 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
2 Lahorte C.M., van de Wiele C., Bacher K., van den Bossche B., Thierens H., van Belle S., Slegers G., Dierckx R.A. (2003). Biodistribution and dosimetry study of 123I-rh-annexin V in mice and humans. Nucl Med Commun.
3 Bohm I., Schild H. (2003). Apoptosis: the complex scenario for a silent cell death. Mol Imaging Biol.
4 Kerr J.F., Wyllie A.H., Currie A.R. (1972). Apoptosis: a basic biological phenomenon with wide-ranging implications in tissue kinetics. Br J Cancer.
5 Brauer M. (2003). In vivo monitoring of apoptosis. Prog Neuropsychopharmacol Biol Psychiatry.
6 Van de Wiele C., Vermeersch H., Loose D., Signore A., Mertens N., Dierckx R. (2004). Radiolabeled annexin-V for monitoring treatment response in oncology. Cancer Biother Radiopharm.
7 Lahorte C.M., Vanderheyden J.L., Steinmetz N., Van de Wiele C., Dierckx R.A., Slegers G. (2004). Apoptosis-detecting radioligands: current state of the art and future perspectives. Eur J Nucl Med Mol Imaging.
8 Narula J., Kietselaer B., Hofstra L. (2004). Role of molecular imaging in defining and denying death. J Nucl Cardiol.
9 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
10 Boersma H.H., Kietselaer B.L., Stolk L.M., Bennaghmouch A., Hofstra L., Narula J., Heidendal G.A., Reutelingsperger C.P. (2005). Past, present, and future of annexin A5: from protein discovery to clinical applications. J Nucl Med.
11 Ke S., Wen X., Wu Q.P., Wallace S., Charnsangavej C., Stachowiak A.M., Stephens C.L., Abbruzzese J.L., Podoloff D.A., Li C. (2004). Imaging taxane-induced tumor apoptosis using PEGylated, 111In-labeled annexin V. J Nucl Med.
12 Wen X., Wu Q.P., Ke S., Ellis L., Charnsangavej C., Delpassand A.S., Wallace S., Li C. (2001). Conjugation with (111)In-DTPA-poly(ethylene glycol) improves imaging of anti-EGF receptor antibody C225. J Nucl Med.
13 Wen X., Wu Q.P., Ke S., Wallace S., Charnsangavej C., Huang P., Liang D., Chow D., Li C. (2003). Improved radiolabeling of PEGylated protein: PEGylated annexin V for noninvasive imaging of tumor apoptosis. Cancer Biother Radiopharm.
14 Wen X., Wu Q.P., Lu Y., Fan Z., Charnsangavej C., Wallace S., Chow D., Li C. (2001). Poly(ethylene glycol)-conjugated anti-EGF receptor antibody C225 with radiometal chelator attached to the termini of polymer chains. Bioconjug Chem.